# ^11^C-BMS-5p and ^18^F-FBzBMS: radiolabeled analogs of BMS-207940, a potent and selective antagonist of endothelin receptor subtype A

Chemical name: | ^11^C-BMS-5p and ^18^F-FBzBMS: radiolabeled analogs of BMS-207940, a potent and selective antagonist of endothelin receptor subtype A
Abbreviated name: | [^11^C]-BMS-5p and [^18^F]FBzBMS
Synonym:
Agent Category: | Compound
Target: | Endothelin receptor subtype A (ET_A_)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the structure of [^18^F]FBzBMS above for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=endothelin&cmd=DetailsSearch)]

The endothelin (ET) family consists of three isoform peptides, ET-1 (22 amino acids (aa)), ET-2 (23 aa), and ET-3 (27 aa), that mediate their activity through two G-protein–coupled ET receptors (ETR) designated as A (ET_A_) and B (ET_B_) (1). Each isoform of ET has a distinct receptor affinity and physiological activity. ET_A_ is located primarily on the smooth muscle cells and has a high affinity for the ET-1 and ET-2 peptides. ET_B_ has an affinity for all of the ET peptides and is expressed in several cells types such as epithelial cells, endothelial cells, endocrine cells, and nerve cells (1). Binding of ETs to ET_A_ results in vasoconstriction and the development of hypertension; however, binding of ETs to ET_B_ results in the production of nitric oxide and prostaglandins, which promote vasodilation (1). There is much evidence that ET-1 plays a prominent role in the development of pulmonary hypertension and even heart failure (2). In addition, it is well known that ETs, particularly ET-1, are involved in the growth of cancerous tumors because they promote cell transformation and angiogenesis; an elevated level of ET-1 in the blood indicates a poor prognosis for the patient (3). Because of their involvement in the development of cardiovascular disorders, the United States Food and Drug Administration (FDA) approved the use of small molecule ETR antagonists (http://dailymed.nlm.nih.gov/dailymed/search.cfm?startswith=endothelin+receptor+antagonists&x=17&y=9) for the treatment of these conditions.

It has been shown that radioiodinated (^123/125^I) or ^18^F-labeled ET-1 is suitable for the noninvasive imaging of ETRs in rodents and non-human primates (4). Although radiolabeled small molecule antagonists of ET_A_ have been developed and evaluated in vitro and for the in vivo imaging of ETRs in animals, none of these radiolabeled compounds has been used for the imaging of this receptor in humans (4). In a continuing effort to develop ET_A_ antagonists, Murugesan et al. showed that BMS-207904, a biphenyl sulfonamide, is a highly potent (K_i_ = 10 pM) antagonist that is 80,000-fold more selective of ET_A_ than of ET_B_ (5). Mathews et al. synthesized ^11^C-labeled and ^18^F-labeled analogs of BMS-207904, designated as [^11^C]-BMS-5p and [^18^F]FBzBMS, and studied the biodistribution of these radiolabeled antagonists in normal mice (4). The tracers were also evaluated for the imaging of ET_A_ with positron emission tomography (PET) in a baboon (4). In another study, [^18^F]FBzBMS was used with PET to assess the in vivo expression of ET_A_ in healthy and infarcted rat hearts (6).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Endothelin+receptor+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Endothelin+receptors&Search=Search) related to endothelin receptors

Endothelin receptors in Online Mendelian Inheritance in Man Database (OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=Endothelin+receptors))

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_001948.1) sequence of a precursor of human endothelin-1 receptor isoform

Human endothelin receptor subtype A, transcript variant 2, mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_001166055.1) sequence

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBzBMS%20synthesis&cmd=DetailsSearch)]

The synthesis of [^11^C]-BMS-5p and [^18^F]FBzBMS has been described by Mathews et al. (4).

[^11^C]-BMS-5p was synthesized in 36 min and had an average radiochemical yield (RCY) of 1.5 ± 0.4% as determined with high-performance liquid chromatography (HPLC). The radiochemical purity (RCP) of [^11^C]-BMS-5p was >99%, with a specific activity (SA) of 1.051 TBq/μmol (28.4 Ci/μmol; n = 5 reactions) at the end of synthesis (4).

The synthesis of [^18^F]FBzBMS was completed in 130 min, and [^18^F]FBzBMS had RCY, RCP, and SA values of 0.54 ± 0.44%, 99%, and 12.9 GBq/μmol (349 mCi/μmol; n = 7 reactions), respectively, at the end of synthesis (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBzBMS%20in%20vitro%20studies&cmd=DetailsSearch)]

The 50% inhibitory concentrations (IC_50_) of BMS-207940, nonradioactive BMS-5p, and nonradiactive FBzBMS for ET_A_ were determined with a mixture of human kidney cortex and medulla cell membranes (4). [^125^I]-ET was used as the receptor ligand for this assay. The IC_50_ values of BMS-207940, BMS-5p, and FBzBMS were reported to be 4.73 nM, 14.26 nM, and 3.09 nM, respectively.

The in vivo stability of the two tracers was determined in healthy mice (n = 4 animals) (4). The rodents were given an intraperitoneal injection of either 37 MBq (1 mCi) [^11^C]-BMS-5p or 7.4 MBq (0.2 mCi) [^18^F]FBzBMS, and blood was collected from the animals at various time points (4). HPLC analysis of plasma isolated from the various blood samples showed that only 14% of [^11^C]-BMS-5p was metabolized at 25 min p.i. compared with 8.5% of [^18^F]FBzBMS at 40 min p.i. A similar study with a baboon showed that ~36% of both [^11^C]-BMS-5p and [^18^F]-FBzBMS were metabolized in the plasma by 90 min p.i.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBzBMS%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]-BMS-5p and [^18^F]FBzBMS was studied in healthy mice (4). The animals (n = 3 mice/tracer) were injected with either 11.3 MBq (306 μCi, 0.2 μg/kg body weight (BW)) [^11^C]-BMS-5p or 2.7 MBq (72 μCi, 2.55 μg/kg BW) [^18^F]FBzBMS through the tail vein, and the rodents were euthanized at preselected time points to retrieve the organs of interest. The amount of radioactivity accumulated in the different tissues was determined and presented as percent of injected dose per gram tissue (% ID/g; Table 1). With both radiochemicals, maximum uptake of radioactivity was observed in the liver, followed by lungs and heart at all of the time points. The liver showed a higher accumulation of label with [^18^F]FBzBMS than with [^11^C]-BMS-5p during the entire course of the study. All other organs showed a constant level of radioactivity at all of the time points.

To determine the ET_A_ binding specificity of [^11^C]-BMS-5p and [^18^F]FBzBMS, the mice (n = 3 animals/labeled compound) were given an intravenous injection of BMS-207940 (1 mg/kg BW) 5 min before administration of the labeled compounds (4). At 60 min p.i., the animals were euthanized and treated as described above to determine the amount of radioactivity accumulated in the various tissues. The lungs and the kidneys showed >64% specific binding of label with both radiotracers. The heart showed 63% and 81% specific uptake of radioactivity with [^11^C]-BMS-5p and [^18^F]FBzBMS, respectively.

In another study, [^18^F]FBzBMS was evaluated with PET imaging to determine the level of ET_A_ expression in healthy and injured rat hearts (injury induced by myocardial infarction) (6). In vivo blocking studies with BMS-207940 and bosentan (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=749e42fb-2fe0-45dd-9268-b43bb3f4081c) (an oral ETR antagonist approved by the FDA for the treatment of pulmonary hypertension) confirmed that the tracer can be used with PET to visualize the expression of ETR in these rodents. In addition, it has been shown that [^18^F]FBzBMS can be used with PET to compare the expression of ETR in the hearts of healthy rats (n = 5 animals) and the infarcted hearts of the animals (n = 32 rats).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBzBMS%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBzBMS%20Non-Human%20Primates&cmd=DetailsSearch)]

[^11^C]-BMS-5p and [^18^F]FBzBMS were evaluated for the noninvasive imaging of ET_A_ in a non-human primate (4). For this, a baboon (Papio anubis; under anesthesia) was injected intravenously with either 292 ± 25 MBq (7.88 ± 0.68 mCi, 0.22 ± 0.01 μg) [^11^C]-BMS-5p or 158 ± 12 MBq (4.28 ± 0.33 mCi, 9.82 ± 3.15 μg) [^18^F]FBzBMS, and PET images of the animal's heart were acquired for up to 90 min p.i (4). Subsequently regions of interest were drawn around the myocardium and the lungs on the PET images, and time-activity curves for the organs were generated. At all of the time points, a high uptake of radioactivity was observed in the myocardium compared with the lungs with both tracers. With both radioligands, the heart/blood label uptake ratio was reported to be 4.7 between 35 min p.i. and 85 min p.i. For blocking studies, the animal was pretreated with 1 mg/kg BW BMS-207940, and both tracers exhibited specific binding of 85% in the heart at 85 min p.i. From this study, the investigators concluded that both [^11^C]-BMS-5p and [^18^F]FBzBMS are suitable for the detection and characterization of ET_A_ in the non-human primates (4).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBzBMS%20Human%20Studies&cmd=DetailsSearch)]

No information is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some of the studies reported in this chapter were supported by National Institutes of Health grants CA115532, DK50183, CA092871, and CA103175.

## References

1 Ohkita M., Tawa M., Kitada K., Matsumura Y. (2012). Pathophysiological roles of endothelin receptors in cardiovascular diseases. J Pharmacol Sci.
2 Barton M., Yanagisawa M. (2008). Endothelin: 20 years from discovery to therapy. Can J Physiol Pharmacol.
3 Said N., Theodorescu D. (2012). Permissive role of endothelin receptors in tumor metastasis. Life Sci.
4 Mathews W.B., Murugesan N., Xia J., Scheffel U., Hilton J., Ravert H.T., Dannals R.F., Szabo Z. (2008). Synthesis and in vivo evaluation of novel PET radioligands for imaging the endothelin-A receptor. J Nucl Med.
5 Murugesan N., Gu Z., Spergel S., Young M., Chen P., Mathur A., Leith L., Hermsmeier M., Liu E.C., Zhang R., Bird E., Waldron T., Marino A., Koplowitz B., Humphreys W.G., Chong S., Morrison R.A., Webb M.L., Moreland S., Trippodo N., Barrish J.C. (2003). Biphenylsulfonamide endothelin receptor antagonists. 4. Discovery of N-[[2'-[[(4,5-dimethyl-3-isoxazolyl)amino]sulfonyl]-4-(2-oxazolyl)[1,1'-biphenyl] - 2-yl]methyl]-N,3,3-trimethylbutanamide (BMS-207940), a highly potent and orally active ET(A) selective antagonist. J Med Chem.
6 Higuchi T., Rischpler C., Fukushima K., Isoda T., Xia J., Javadi M.S., Szabo Z., Dannals R.F., Mathews W.B., Bengel F.M. (2013). Targeting of Endothelin Receptors in the Healthy and Infarcted Rat Heart Using the PET Tracer 18F-FBzBMS. J Nucl Med.

Table 1: Biodistribution of radioactivity from [^11^C]-BMS-5p and [^18^F]FBzBMS in healthy mice (4).

Organ | [ ^ 11 ^ C]-BMS-5p | | | | [ ^ 18 ^ F]FBzBMS
Organ | Time p.i. (min)
Organ | 5 | 30 | 90 | 120 | 5 | 30 | 90 | 120
Liver | 43.46 ± 4.99 | 20.72 ± 0.37 | 13.43 ± 0.74 | NA | 62.70 ± 1.26 | 44.66 ± 8.14 | 23.37 ± 2.67 | 12.95 ± 2.36
Lungs | 9.22 ± 1.40 | 7.50 ± 0.54 | 7.16 ± 0.82 | NA | 3.76 ± 0.29 | 5.80 ± 1.01 | 5.89 ± 0.98 | 5.09 ± 2.16
Heart | 5.07 ± 0.27 | 2.82 ± 0.29 | 3.42 ± 0.51 | NA | 2.37 ± 0.11 | 3.07 ± 0.08 | 3.05 ± 0.02 | 3.08 ± 0.68
Kidney | 9.15 ± 1.55 | 3.93 ± 0.18 | 2.59 ± 0.37 | NA | 8.42 ± 1.39 | 4.67 ± 1.00 | 3.02 ± 0.12 | 1.83 ± 0.62
Blood | 12.91 ± 0.38 | 5.17 ± 3.41 | 1.12 ± 0.20 | NA | 3.44 ± 0.27 | 1.85 ± 0.34 | 0.61 ± 0.05 | 0.40 ± 0.12

NA, not available; p.i., postinjection. Data are presented as % injected dose per gram (ID/g). For complete data, see Mathews et al. (4).